# Gallium-68-dotamaleimide-Cys165-annexin A5

Chemical name: | Gallium-68-dotamaleimide-Cys165-annexin A5
Abbreviated name: | ^68^Ga-Cys165-AnxA5
Synonym:
Agent Category: | Proteins
Target: | Phosphatidylserine
Target Category: | Lipids
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | Gallium-68 (^68^Ga)
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=tumor%20responses%20and%20molecular%20imaging)]

The gallium-68 (^68^Ga)-dotamaleimide-Cys165-annexin A5 (AnxA5) conjugate, abbreviated as ^68^Ga-Cys165-AnxA5, is a radionuclide agent developed by Bauwens et al. for phosphatidylserine (PS)-targeted positron emission tomography (PET) of tumor cell apoptosis after chemotherapy and radiotherapy (1). ^68^Ga has a half-life of 68 min and emits positrons with E_max_ β^+^ = 1.9 MeV.

Evaluation of tumor response to therapy is traditionally based on volumetric and morphological changes before and after treatment (2); these changes, however, occur rather late after effective therapy. Recent studies have shown that successful treatment induces apoptosis of tumor cells at the very early stage, and externalization of PS is one of the earliest events in apoptosis (3, 4). PS is a membrane phospholipid normally restricted to the inner leaflet of the lipid bilayer. Within a few hours of the apoptotic stimulus, however, PS externalizes to the outer leaflet of the cell membrane and is readily accessible to exogenous molecules. These findings indicate that the early response of tumors to therapy can be evaluated by detection of apoptosis via imaging of externalized PS (2, 3, 5).

AnxA5 is a cellular protein of 36 kDa and specifically binds to membrane-bound PS with nanomolar affinity in the presence of calcium (Ca^2+^) (3, 6, 7). AnxA5 has no immunogenicity or toxicity when used in vivo. These features of AnxA5 make it a valuable agent for in vivo apoptosis detection. AnxA5 was first radiolabeled with ^125^I and later with other radionuclides, including ^99m^Tc, ^18^F, ^111^In, and ^68^Ga (1, 5, 6). Both preclinical and clinical studies have shown that AnxA5-based radionuclides are promising tracers for the rapid dection of apoptosis. However, there are several issues that remain to be resolved (1, 2). First is the suboptimal pharmacokinetics of radiolabeled AnxA5 agents. A high nonspecific accumulation is often observed in the liver and kidneys. Second is the decreased binding affinity caused by radiolabeling and other conjugations. Optimal binding of AnxA5 to PS also requires a micromolar concentration of Ca^2+^. Third is the inability of AnxA5 agents to differentiate apoptosis from necrosis because PS is also externalized during necrosis.

To maintain the binding affinity of AnxA5, Tait et al. applied a site-specific labeling technique in the radiolabeling of AnxA5, and they have shown that specific labeling in the non-binding region of AnxA5 improves the detection of apoptosis compared to random labeling of amino residues (8). Using a similar method, Bauwens et al. synthesized two radionuclide agents, ^68^Ga-Cys2-AnxA5 and ^68^Ga-Cys165-AnxA5 (1). Cys2-AnxA5 and Cys165-AnxA5 are two variants of AnxA5, and they contain a single available Cys residue at the 2-position and at the 165-position, respectively. Both Cys residues are located at the concave side of AnxA5, opposite the convex side that harbors the Ca^2+^/PS binding sites. Covalent coupling of large structures such as liposomes and iron nanoparticles via thiol-chemistry to the Cys2-AnxA5 or Cys165-AnxA5 exhibits no side effect on the PS binding activity (8-11). Bauwens et al. showed that both ^68^Ga-Cys2-AnxA5 and ^68^Ga-Cys165-AnxA5 exhibit a clear binding to apoptotic cells and are promising tracers for the rapid evaluation of cancer therapy (1). No significant differences between the two analogs were observed in the data obtained from in vitro and in vivo analyses. This chapter summarizes the data obtained with ^68^Ga-Cys165-AnxA5, and another chapter in MICAD summarizes the data obtained with ^68^Ga-Cys2-AnxA5.

### Related Resource Links:

- Annexin-based chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=annexin%20AND%20micad%5bbook%5d)
- Protein information of annexins (http://www.ncbi.nlm.nih.gov/protein?term=Annexin)
- Structures of annexins (http://www.ncbi.nlm.nih.gov/structure?term=Annexin)
- Annexin-related compounds in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance?term=Annexin)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=21492787)]

Bauwens et al. described the synthesis of ^68^Ga-Cys165-AnxA5 in detail (1). ^68^Ga was obtained from a titanium dioxide–based ^68^Ge/^68^Ga generator, and ^68^Ga-dotamaleimide was synthesized by heating a mixture of ^68^Ga and dotamaleimide for 8 min at 90°C. Cys165-AnxA5 was produced by site-directed mutagenesis of human AnxA5 cDNA and expressed in Escherichia coli (purity >95%). The introduction of Cys165 did not affect the Ca^2+^-dependent PS binding. To couple with ^68^Ga-dotamaleimide, Cys165-AnxA5 was treated with dithiothreitol to convert all potentially formed disulfide bridges to free thiols. The ^68^Ga-dotamaleimide and AnxA5 variant were then mixed, incubated for 15 min at 37°C, and purified. This step resulted in a coupling yield (radiochemical yield) of 70 ± 10%. Purification led to a loss of ~10%; the radiochemical purity was >98%. The total synthesis time was ~55 min, with an end-of-synthesis yield of 25% (43% decay-corrected). ^68^Ga-Cys165-AnxA5 was stable for at least 1.5 h in vitro in HEPES buffer and in plasma, both at 25°C and at 37°C. No free ^68^Ga, ^68^Ga-dotamaleimide, or any other metabolites could be detected.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=21492787)]

The in vitro binding capacity of ^68^Ga-Cys165-AnxA5 was evaluated with Jurkat cells after anti-Fas treatment (1). Jurkat cells have been shown to expose PS upon treatment with anti-Fas (12). The total activity bound to anti-Fas–treated Jurkat cells (70.1 ± 16.7%) was approximately five times higher than the total activity bound to untreated cells (13.4 ± 2.7%), indicating a well-preserved PS binding capacity. No blocking studies were reported.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=21492787)]

Dynamic PET imaging was first performed in healthy Naval Medical Research Institute (NMRI) mice (n = 4) after tail vein injection of ^68^Ga-Cys165-AnxA5 (7–15 MBq (0.19–0.41 mCi)) (1). Images revealed a fast clearance of the tracer from the blood toward the kidneys, with no significant change in biodistribution from 30 min to 60 min after injection. The blood half-life of ^68^Ga-Cys165-AnxA5 was 5.5 min. Dissection data of the organs confirmed that ^68^Ga-Cys165-AnxA5 was cleared mainly via the urinary tract. A high percentage of activity was retained in the kidneys, in particular in the cortex, with only limited clearance toward the urinary bladder. Analysis of plasma and urine samples indicated that no radioactive metabolites could be detected in the plasma of the animal, whereas activity in the urine was only in the form of radiolabeled metabolites, likely small ^68^Ga-dotamaleimide-Cys adducts. Minor uptake was also observed in the liver, intestines, spleen, and lungs.

Detection of apoptosis with ^68^Ga-Cys165-AnxA5 was performed in anti-Fas–treated animals (n = 4) (1). Anti-Fas monoclonal antibody (mAb) treatment induces apoptosis in normal organs, especially the liver. NMRI mice were pretreated with 0.2 μg/g purified hamster anti-Fas mAb for 90 min, at which time the mice were injected via the tail vein with 7–15 MBq (0.19–0.41 mCi) ^68^Ga-Cys165-AnxA5. Images were obtained at 1 h after injection, and the accumulation in organs was calculated and expressed as a percentage of injected dose per organ (% ID/organ) following dissection. The ^68^Ga-Cys165-AnxA5 showed a major shift of the radioactivity from the kidneys to the apoptotic liver. There was a significant difference in the amount of ^68^Ga-Cys165-AnxA5 in the organs of healthy mice compared with that in the organs of anti-Fas–treated mice: liver, 5.81 ± 0.26 (normal) versus 54.3 ± 8.0 (treated); kidneys, 75.7 ± 1.0 (normal) versus 26.7 ± 6.2 (treated); lungs, 0.40 ± 0.09 (normal) versus 0.82 ± 0.09 (treated); and spleen, 0.61 ± 0.07 (normal) versus 1.82 ± 0.49 (treated). The higher uptake in apoptotic liver tissue was further confirmed with autoradiography of the liver slices dissected 1 h after injection.

The feasibility of ^68^Ga-Cys165-AnxA5 in the detection of apoptosis after chemotherapy and radiotherapy was tested in animals bearing lymphoma xenografts (Daudi, a human B-lymphoblast cell line) (1). Animals were treated with cyclophosphamide (125 mg/kg) 1 day before imaging and then with radiation (10 Gy/tumor) 4–6 h before imaging. Dynamic PET imaging was performed 1 h after injection of 7–15 MBq (0.19–0.41 mCi) ^68^Ga-Cys165-Anx (n = 3). This was done before and after treatment of the animals. PET images showed no clear difference in the biodistribution of ^68^Ga-Cys165-AnxA5 between the healthy and tumor-bearing animals. The uptake in the tumor was minimal, but MRI-PET fusion images demonstrated clear delineation of each tumor. The standardized uptake values (SUV_mean_) were then calculated with the following formula: SUV = measured activity concentration in the tumor (Bq/g) × body weight (g) ÷ injected activity (Bq). The after-therapy SUV values significantly exceeded (P < 0.05) those prior to therapy: 0.143 ± 0.034 versus 0.089 ± 0.027 for SUV_10min_; 0.085 ± 0.013 versus 0.057 ± 0.014 for SUV_30min_; and 0.059 ± 0.007 versus 0.057 ± 0.008 for SUV_60min_. These findings were confirmed with the dissection data at 1 h after injection, which showed that the tumor uptake was significantly higher in the treated animals than in the untreated animals (0.156 ± 0.016% ID/g tissue versus 0.106 ± 0.024% ID/g tissue). Autoradiography of the tumor slices also showed increased activity in the treated tumors. The apoptosis in the tumor tissue seemed very inhomogeneous as several regions showed an uptake 10–20 times higher than the tumor uptake prior to treatment, whereas other regions were relatively unaffected (1).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Bauwens M., De Saint-Hubert M., Devos E., Deckers N., Reutelingsperger C., Mortelmans L., Himmelreich U., Mottaghy F.M., Verbruggen A. (2011). Site-specific 68Ga-labeled Annexin A5 as a PET imaging agent for apoptosis. Nucl Med Biol.
2 Neves A.A., Brindle K.M. (2006). Assessing responses to cancer therapy using molecular imaging. Biochim Biophys Acta.
3 Schutters K., Reutelingsperger C. (2010). Phosphatidylserine targeting for diagnosis and treatment of human diseases. Apoptosis.
4 Nguyen Q.D., Aboagye E.O. (2010). Imaging the life and death of tumors in living subjects: Preclinical PET imaging of proliferation and apoptosis. Integr Biol (Camb).
5 Kapty J., Murray D., Mercer J. (2010). Radiotracers for noninvasive molecular imaging of tumor cell death. Cancer Biother Radiopharm.
6 Kuge Y., Zhao S., Takei T., Tamaki N. (2009). Molecular imaging of apoptosis with radio-labeled Annexin A5 focused on the evaluation of tumor response to chemotherapy. Anticancer Agents Med Chem.
7 Niu G., Chen X. (2010). Apoptosis imaging: beyond annexin V. J Nucl Med.
8 Tait J.F., Smith C., Levashova Z., Patel B., Blankenberg F.G., Vanderheyden J.L. (2006). Improved detection of cell death in vivo with annexin V radiolabeled by site-specific methods. J Nucl Med.
9 De Saint-Hubert M., Mottaghy F.M., Vunckx K., Nuyts J., Fonge H., Prinsen K., Stroobants S., Mortelmans L., Deckers N., Hofstra L., Reutelingsperger C.P., Verbruggen A., Rattat D. (2010). Site-specific labeling of 'second generation' annexin V with 99mTc(CO)3 for improved imaging of apoptosis in vivo. Bioorg Med Chem.
10 van Tilborg G.A., Mulder W.J., Deckers N., Storm G., Reutelingsperger C.P., Strijkers G.J., Nicolay K. (2006). Annexin A5-functionalized bimodal lipid-based contrast agents for the detection of apoptosis. Bioconjug Chem.
11 Li X., Link J.M., Stekhova S., Yagle K.J., Smith C., Krohn K.A., Tait J.F. (2008). Site-specific labeling of annexin V with F-18 for apoptosis imaging. Bioconjug Chem.
12 Green A.M., Steinmetz N.D. (2002). Monitoring apoptosis in real time. Cancer J.